# 2-(3-{1-Carboxy-5-[(6-[^18^F]fluoro-pyridine-3-carbonyl)-amino]-pentyl}-ureido)-pentanedioic acid

Chemical name: | 2-(3-{1-Carboxy-5-[(6-[^18^F]fluoro-pyridine-3-carbonyl)-amino]-pentyl}-ureido)-pentanedioic acid | [image]
Abbreviated name: | [^18^F]DCFPyL | [image]
Synonym: | [^18^F]3 | [image]
Agent Category: | Compounds | [image]
Target: | Prostate-specific membrane antigen (PSMA) | [image]
Target Category: | Antigens | [image]
Method of detection: | Positron emission tomography | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]DCFPyL (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=PSMA+and%20molecular%20imaging)]

2-(3-{1-Carboxy-5-[(6-[^18^F]fluoro-pyridine-3-carbonyl)-amino]-pentyl}-ureido)-pentanedioic acid, abbreviated as [^18^F]DCFPyL, was synthesized by Chen et al. for use in positron emission tomography of tumors expressing prostate-specific membrane antigen (PSMA) (1).

PSMA is a type II transmembrane glycoprotein with three structural domains, including a 19-amino-acid intracellular domain, a 24-amino-acid transmembrane domain, and a large 707-amino-acid extracellular domain (2, 3). Two site-specific carboxypeptidase activities have been assigned to PSMA: N-acetylated α-linked acidic dipeptidase, which hydrolyzes the neuropeptide N-acetyl-aspartyl-glutamate (NAAG) in the brain to regulate release of neurotransmitters, and folate hydrolase activity, which is characterized by the cleavage of terminal glutamates from poly- and gamma-glutamated folates, which play a role in the cellular uptake of dietary folate (2). PSMA has been found to be expressed in the prostate at a level 1,000-fold greater than in other tissues, and many folds higher in prostate cancer tumors than in normal and benign prostate tissues (4, 5). High-grade hormone-sensitive and hormone-insensitive tumors have the greatest PSMA expression. PSMA is also consistently and abundantly expressed on the neovascular endothelium in a wide variety of human solid tumors, but not in blood vessels in normal tissues. These features of PSMA make it an optimal target for developing imaging and therapy strategies for prostate cancer (6).

Besides antibodies and antibody fragments, low molecular weight compounds have also been intensively tested as PSMA inhibitors and as PSMA-targeted imaging agents (1, 6). These compounds can be largely classified into two types: ureas and phosphoramidates (1). Both types of compounds possess a terminal glutamate at the P1' position, which enables productive binding with PSMA. They are also amenable to modification with bulky substituents that interact with the arginine patch or tunnel region on PSMA. Investigators have synthesized a series of ureas, including [^18^F]DCFBC, [^18^F]DCFPyL, and [^111^In]3 (1, 7, 8). [^111^In]3 is a bivalent compound that was synthesized by incorporating a PSMA-binding Lys-Glu urea motif for exploiting click chemistry and a second lysine residue for subsequent modification with an imaging or therapeutic moiety (8). Studies have shown that these radiolabeled PSMA inhibitors have desirable properties as imaging agents for prostate cancer imaging in animal models (1, 7, 8). This chapter summarizes the data obtained with [^18^F]DCFPyL. In another chapter, the data obtained with [^111^In]3 are summarized. The data obtained with [^18^F]DCFBC can be reviewed in the chapter on [^18^F]DCFBC (http://www.ncbi.nlm.nih.gov/books/NBK23394/) in MICAD.

### Related Resource Links:

- PSMA-targeted imaging agents (http://www.ncbi.nlm.nih.gov/books/?term=PSMA+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/gene/2346))
- Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://www.ncbi.nlm.nih.gov/omim/600934))
- PSMA-related clinical trials (http://www.clinicaltrials.gov/ct2/results?term=PSMA&Search=Search) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%5b18F%5dDCFPyL)]

Chen et al. described the synthesis of [^18^F]DCFPyL in detail (1). The tosylate salt of 2-{3-[1-p-methoxybenzylcarboxylate-(5-aminopentyl)]-ureido}-di-p-methoxybenzyl pentanedioate (compound 1) was synthesized, and then compound 1 was reacted with 6-fluoronicotinic acid 2,3,5,6-tetrafluorophenyl ester to generate fluoropyridyl urea (65% yield, compound 2). Deprotection produced 2-(3-{1-carboxy-5-[(6-fluoro-pyridine-3-carbonyl)-amino]-pentyl}-ureido)-pentanedioic acid (compound 3, DCFPyL), with 81% yield. The ^18^F-labeled prosthetic group 6-fluoro-nicotinic acid 2,3,5,6-tetrafluoro-phenyl ester was used to generate [^18^F]DCFPyL.

The radiochemical yields of [^18^F]DCFPyL were 36%–53% based on starting [^18^F]F− (n = 3), with absolute yields of 285–385 MBq (7.7–10.4 mCi) after purification. The mean synthesis time was 128 min from the time of addition of [^18^F]F−. With the addition of 1,628–2,257 MBq (44–61 mCi) [^18^F]F−, the specific radioactivity of [^18^F]DCFPyL was 12.6–17.8 GBq/μmol (340–480 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%5b18F%5dDCFPyL)]

The PSMA enzyme inhibition potency of compound 3 was determined with a modified Amplex Red glutamic acid assay after incubation with the cell lysates of LNCaP cell extracts in the presence of NAAG for 2 h at 37°C (1, 6). The enzyme inhibitory constant (K_i_) for compound 3 was 1.1 ± 0.1 nmol/L, comparable with that of ZJ-43, which was 1.4 ± 0.2 nmol/L under same measurement conditions. ZJ-43 is a urea-based potent inhibitor of NAAG and is used as an internal reference in the assay.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%5b18F%5dDCFPyL)]

Biodistribution of [^18^F]DCFPyL was determined at 30, 60, 120, and 240 min after tail vein injection of 3.7 MBq (0.1 mCi) [^18^F]DCFPyL to nonobese diabetic severe-combined immunodeficient (NOD-SCID) mice that carried both PSMA-positive PC3-PIP and PSMA-negative PC3-flu xenografts (n = 4 mice/group) (1). The percentage of injected dose per gram tissue (% ID/g) was measured ex vivo in selected organs (Table 1). [^18^F]DCFPyL showed a PSMA-dependent uptake, reaching a value of 46.7 ± 5.8% ID/g at 30 min in PC3-PIP xenografts, which decreased by only ~10% over the 4-h period of study. The uptake ratio of PC3-PIP/PC3-flu tumors ranged from 40:1 to >1,000:1. An explanation for the increased tumor uptake of [^18^F]DCFPyL over time could be due to PSMA-mediated internalization within tumor cells. At 60 min after injection, the kidney, liver, and spleen displayed the highest uptake among organs. Rapid clearance from the kidneys was observed, decreasing from 74.1 ± 6.6% ID/g at 30 min to 7.4 ± 0.9% ID/g at 4 h after injection. Relatively low bone uptake (<1% ID/g at all time points) suggests little metabolic defluorination of the [^18^F]DCFPyL.

Table 1: Biodistribution of [^18^F]DCFPyL in selected organs (percent of ID/g) in tumor-bearing mice.

Organ | 30 min | 60 min | 120 min | 240 min
Blood | 1.53 ± 0.19 | 0.24 ± 0.05 | 0.43 ± 0.37 | 0.03 ± 0.01
Liver | 3.88 ± 0.74 | 2.87 ± 0.92 | 2.14 ± 0.11 | 1.80 ± 0.39
Kidney | 74.1 ± 6.6 | 42.3 ± 19.0 | 15.7 ± 3.3 | 7.42 ± 0.89
Bone | 0.82 ± 0.16 | 0.42 ± 0.15 | 0.33 ± 0.08 | 0.43 ± 0.06
Bladder (empty) | 18.6 ± 18.1 | 9.88 ± 4.92 | 6.44 ± 4.42 | 1.54 ± 1.79
PC3-PIP | 46.7 ± 5.8 | 44.2 ± 9.7 | 39.4 ± 5.4 | 36.6 ± 4.3
PC3-Luc | 1.17 ± 0.41 | 0.36 ± 0.14 | 0.11 ± 0.02 | 0.03 ± 0.01
PC3-PIP/PC3-Luc | 40 | 123 | 358 | 1,220

PET/computed tomography was performed after tail vein injection of 14.1 MBq (0.38 mCi) [^18^F]DCFPyL into one NOD-SCID mouse that carried both PSMA-positive PC3-PIP and PSMA-negative PC3-flu xenografts (1). Successive whole-body images were acquired in two bed positions. The dwell time at each position was 1 min, such that a given bed position (or mouse organ) was revisited every 3 min. Imaging showed intense radiochemical uptake only in the kidneys and PC3-PIP tumor after administration of [^18^F]DCFPyL. By 3.5 h after injection, only the PC3-PIP tumor was visible with no radiochemical background in liver or the gastrointestinal tract to obscure potential metastases. No blocking studies were performed in either experiments, but the tumors with and without PSMA support specific tumor binding.

The human dosimetry values were obtained based on the mouse biodistribution data (1). The mouse organ activity concentrations in % ID/g were converted to the human % ID/organ by setting the ratio of organ % ID/g to whole-body % ID/g in the mouse equal to that in humans. The conversion showed that the organ with the highest mean absorbed dose per unit administered activity was the urinary bladder wall (0.15 mGy/MBq), followed by the kidneys (0.05 mGy/MBq). The effective dose based on the International Commission on Radiological Protection 60 (ICRP 60) tissue weighting factors was 13.6 μSv/MBq. A maximum of 331 MBq (9 mCi) could be administered without exceeding the 50-mGy critical organ dose limit (urinary bladder wall in this case) for a single administration of radioactive material for research use as specified in Code of Federal Regulations 21, part 361.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Chen Y., Pullambhatla M., Foss C.A., Byun Y., Nimmagadda S., Senthamizhchelvan S., Sgouros G., Mease R.C., Pomper M.G. (2011). 2-(3-{1-Carboxy-5-[(6-[18F]fluoro-pyridine-3-carbonyl)-amino]-pentyl}-ureido)-pen tanedioic acid, [18F]DCFPyL, a PSMA-based PET imaging agent for prostate cancer. Clin Cancer Res.
2 Conway R.E., Petrovic N., Li Z., Heston W., Wu D., Shapiro L.H. (2006). Prostate-specific membrane antigen regulates angiogenesis by modulating integrin signal transduction. Mol Cell Biol.
3 Foss C.A., Mease R.C., Cho S.Y., Kim H.J., Pomper M.G. (2012). GCPII imaging and cancer. Curr Med Chem.
4 Olson W.C., Heston W.D., Rajasekaran A.K. (2007). Clinical trials of cancer therapies targeting prostate-specific membrane antigen. Rev Recent Clin Trials.
5 Denmeade, S.R., Mhaka, A.M., Rosen, D.M., Brennen, W.N., Dalrymple, S., Dach, I., Olesen, C., Gurel, B., Demarzo, A.M., Wilding, G., Carducci, M.A., Dionne, C.A., Moller, J.V., Nissen, P., Christensen, S.B., and Isaacs, J.T. Engineering a prostate-specific membrane antigen-activated tumor endothelial cell prodrug for cancer therapy. Sci Transl Med. 2012: 4(140): 140ra86.
6 Chen Y., Foss C.A., Byun Y., Nimmagadda S., Pullambhatla M., Fox J.J., Castanares M., Lupold S.E., Babich J.W., Mease R.C., Pomper M.G. (2008). Radiohalogenated prostate-specific membrane antigen (PSMA)-based ureas as imaging agents for prostate cancer. J Med Chem.
7 Mease R.C., Dusich C.L., Foss C.A., Ravert H.T., Dannals R.F., Seidel J., Prideaux A., Fox J.J., Sgouros G., Kozikowski A.P., Pomper M.G. (2008). N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-4-[18F]fluorobenzyl-L-cysteine, [18F]DCFBC: a new imaging probe for prostate cancer. Clin Cancer Res.
8 Banerjee S.R., Pullambhatla M., Shallal H., Lisok A., Mease R.C., Pomper M.G. (2011). A modular strategy to prepare multivalent inhibitors of prostate-specific membrane antigen (PSMA). Oncotarget.